# ^186^Re-Labeled [N-[2[[3-(3,3-diphosphonopropylcarbamoyl)propyl]-2-thioethylamino]acetyl]-2-aminoethylenethiolate] oxorhenium (V)

Chemical name: | ^186^Re-Labeled [N-[2[[3-(3,3-diphosphonopropylcarbamoyl)propyl]-2-thioethylamino]acetyl]-2-aminoethylenethiolate] oxorhenium (V)
Abbreviated name: | [^186^Re]MAMA-BP
Synonym:
Agent Category: | Compound
Target: | Hydroxyapatite: Bone imaging Molecular target: Farnesyl disphosphate (pyrophosphate) synthase
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^186^Re
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^186^Re]MAMA-BP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipycolylamine%20alendronate&cmd=DetailsSearch)]

Bisphosphonates (BPs) or nitrogen-containing bisphosphonates (NBPs) are often used for the management of pain palliation and disorders related to skeletal tissue, including those arising from cancer metastases, because these compounds have a very high affinity for hydroxyapatite (HA), a component of the bone matrix. These phosphonates or their derivatives tend to accumulate in osteoclasts located at areas of increased bone metabolism by inhibiting the enzyme farnesyl diphosphate (or pyrophosphate) synthase, an important regulatory enzyme of the cellular mevalonate pathway, which is involved in protein prenylation (1). The molecular mechanism of action of BPs and the NBPs has been described by Drake et. al. (2). Several BPs and NBPs are commercially available for clinical use to treat different bone disorders, and there are ongoing clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) approved by the United States Food and Drug Administration to evaluate these compounds for the treatment of various bone ailments. In addition, BPs are often labeled with ^99m^Tc or ^186/188^Re and used for the imaging and treatment of pain as a result of bone metastases from cancer such as that of the breast or the prostate (3). However, these compounds have limited efficacy primarily because they exist either as a mixture of anionic compounds with varying properties (e.g., ^99m^Tc- labeled methyl diphosphonate (MDP)) or are unstable (e.g., ^86^Re-labeled 1-hydroxyethylidene-1,1-diphosphonate) under in vivo conditions, resulting in a reduced uptake at targeted bone areas and an increased accumulation in non-target soft tissue such as the gastric lining of the stomach (4). The limited clinical utility of radiolabeled BPs was suggested to be caused by the dual activities exhibited by the compounds: one phosphonate group acts as a radionuclide chelator, and the other phosphonate group binds to the target(s).Therefore, due to the close proximity of the two groups, one activity may be interfering with the other (4).

In an effort to solve the stability problems observed with the ^186^Re-labeled NBPs, Ogawa et al. developed two new NBPs, ^186^Re-[N-[2-[[3-(3,3-diphosphonopropylcarbamoyl)propyl]-2-thioethylamino]acetyl]-2-aminoethylenethiolate] oxorhenium (V) ([^186^Re]MAMA-BP) and its hydroxylated derivative, ^186^Re-[N-[2-[[4-[(4-hydroxy-4,4-diphosphonobutyl)amino]-4-oxobutyl]-2-thioethylamino]acetyl]-2-aminoethanethiolate] oxorhenium (V) ([^186^Re]MAMA-HBP) (3). The investigators then compared the two compounds for their affinity to HA under in vitro conditions and studied the biodistribution of the radiochemicals in normal mice. This chapter presents the results obtained with [^186^Re]MAMA-BP. Results obtained with [^186^Re]MAMA-HBP are presented in a separate chapter of MICAD (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20synthesis&cmd=DetailsSearch)]

A ^186^Re-glucoheptonate ligand exchange reaction was used for the synthesis of [^186^Re]MAMA-BP and ^186^Re-1-hydroxyethylidene-1,1-diphosphonate ([^186^Re]-MAMA-HEDP; used as a control in the various studies) and is detailed elsewhere (6). The radiochemical yield of [^186^Re]MAMA-BP was reported to be between 21.3 ± 4.5 and 32.0 ± 4.1% with a purity of 96.4 ± 1.4%. Specific activity of the radiolabeled compounds was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20in%20vitro%20stability&cmd=DetailsSearch)]

The in vitro stability of [^186^Re]MAMA-BP after a 24-h incubation in 0.1 M phosphate-buffered saline (pH, 7.0) saturated with 95% O_2_ and 5% CO_2_ at 37°C was reported to be 81.8 ± 1.7% as determined with reversed-phase high-performance liquid chromatography or thin-layer chromatography. Under the same conditions, the stability of [^186^Re]MAMA-HBP was reported to be 75.55 ± 1.57%.

The HA binding of [^186^Re]MAMA-BP was determined by using different amounts (1–25 mg/mL) of commercially available HA beads suspended in Tris/HCl-buffered saline (pH, 7.4) as described by Ogawa et al. (3). The percent of HA binding was determined with an equation given elsewhere (3). Approximately 40% of [^186^Re]MAMA-BP bound to the HA beads at the lowest concentration (compared with ~70% for [^186^Re]MAMA-HBP) and increased to ~95.0% at the highest concentration (compared with ~97.5% for [^186^Re]MAMA-HBP). Results from this study indicated that [^186^Re]MAMA-HBP had a higher affinity for HA than [^186^Re]MAMA-BP.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^186^Re]MAMA-BP and [^186^Re]MAMA-HBP was investigated in normal, male ddY mice after intravenous administration of the respective labeled compounds (3). For this study, another NBP, [^186^Re]HEDP, was used as a control. The animals (n = 5–6 mice per time point) were euthanized at designated time points ranging from 10 min to 24 h postinjection (p.i.). Organs of interest (liver, kidney, blood, intestine, stomach, and the complete left femur) were removed from the cadavers and weighed, and the amount of radioactivity accumulated in the tissues was measured, and the data were presented as percent injected dose per gram tissue (% ID/g).

The tissue distribution pattern of radioactivity from [^186^Re]MAMA-BP was reported to be similar to that observed with [^186^Re]MAMA-HBP and [^186^Re]MAMA-HEDP (3). Maximum label was deposited on the femur at all time points with the radiochemicals (21.38 ± 3.83% ID/g with [^186^Re]MAMA-BP, 24.80 ± 2.41% ID/g with [^186^Re]MAMA-HBP, and 13.09 ± 2.90% ID/g with [^186^Re]MAMA-HEDP) at 24 h p.i., followed by the kidneys (varying from 2.43 ± 0.53% ID/g with [^186^Re]MAMA-BP to 0.42 ± 0.10% ID/g with [^186^Re]MAMA-HEDP) at the same time point. The femur/blood ratios of radioactivity were ~1,200 with [^186^Re]MAMA-HBP compared with ~800 and ~400 with [^186^Re]MAMA-BP and [^186^Re]MAMA-HEDP, respectively. In addition, the blood clearance of radioactivity from [^186^Re]MAMA-HEDP was slower than that of the other two ^186^Re-labeled MAMA-bisphosphonates, and it had a lower accumulation in the liver.

Ogawa et al. calculated the radiation dose estimates for the three bisphosphonates for adult patients by monoexponential extrapolation of the biodistribution data (3). Although the red-marrow/bone-surface and total-body/bone-surface ratios for all the radiolabeled compounds were the same, the effective-dose/bone-surface ratio of [^186^Re]MAMA-HEDP was higher than that of either [^186^Re]MAMA-BP or [^186^Re]MAMA-HBP.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonates%20non%20primate%20mammal%20studies&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonates%20non%20human%20primate%20studies&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
2 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
3 Ogawa K., Mukai T., Arano Y., Otaka A., Ueda M., Uehara T., Magata Y., Hashimoto K., Saji H. (2006). Rhemium-186-monoaminemonoamidedithiol-conjugated bisphosphonate derivatives for bone pain palliation. Nucl Med Biol.
4 Torres Martin de Rosales R., Finucane C., Mather S.J., Blower P.J. (2009). Bifunctional bisphosphonate complexes for the diagnosis and therapy of bone metastases. Chem Commun (Camb).
5 Chopra, A., 186Re-Labeled [N-2[[4-[(4-hydroxy-4,4-diphosphonobutyl)amino]-4-oxobutyl]-2-thioethylamino]acetyl]-2-aminoethylenethiolate] conjugated to hydroxyl-bisphosphonate. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
6 Ogawa K., Mukai T., Arano Y., Hanaoka H., Hashimoto K., Nishimura H., Saji H. (2004). Design of a radiopharmaceutical for the pallation of painful bone metastases: rhenium-186-labeled bisphosphonate derivative. J. Label. Compd. Radiopharm.